# 2-(3-Fluoro-[4-^11^C]tolyl)-4,5-dihydro-1H-imidazole

Chemical name: | 2-(3-Fluoro-[4-^11^C]tolyl)-4,5-dihydro-1H-imidazole
Abbreviated name: | [^11^C]FTIMD
Synonym:
Agent category: | Compound
Target: | I_2_-imidazoline receptor (I_2_R)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20FTIMD)]

Two major imidazoline binding sites (I_1_R and I_2_R) have been identified (1, 2). The I_1_R and I_2_R exhibit high affinities for clonidine and idazoxan, respectively. Clonidine and its analogs mediate effects independent of α_2_-adrenoceptor at the IR receptors. IR receptors are widely distributed in the central and peripheral nervous systems and in various organs such as the pancreas, liver, kidney, lung, and heart (3-6). I_1_R is associated with hypertension (7), whereas I_2_R is associated with depression (8), Alzheimer’s disease (9), Parkinson’s disease (10), Huntington’s disease (10), and glial cell tumors (11). High densities of I_2_R have been observed in the arcuate nucleus, interpeduncular nucleus, pineal gland, and ventricles in human brain (12). The I_2_R gene has not been identified. Tesson et al. (13) showed that I_2_R is localized to the mitochondrial outer membrane of the human and rabbit liver. Anastassiadou et al. (14) showed that 2-(3-fluoro-4-tolyl)-4,5-dihydro-1H-imidazole (FTIMD) has a high and selective affinity for I_2_R. Kawamura et al. (15) evaluated [^11^C]FTIMD as a positron emission tomography (PET) agent for the noninvasive study of I_2_R in the brain and peripheral organs.

### Related Resource Links:

- Chapters in MICAD (Imidazoline receptors (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=Imidazoline%5BAll+Fields%5D+AND+micad%5Bbook%5D))
- Gene information in NCBI (I_1_R (http://www.ncbi.nlm.nih.gov/gene/11188), α_2_-adrenoceptors (http://www.ncbi.nlm.nih.gov/gene?term=alpha%20adrenoceptor%20human))
- Articles in Online Mendelian Inheritance in Man (OMIM) (I_1_R (http://omim.org/entry/601174), α_2_-adrenoceptors (http://omim.org/search?index=entry&start=1&limit=10&search=alpha-2-adrenergic+receptor&sort=score+desc+%2C+prefix_sort+desc&sort=score+desc+%2C+prefix_sort+desc))
- Clinical trials (Clonidine (http://www.clinicaltrials.gov/ct2/results?term=clonidine))
- Drug information in FDA (Clonidine (http://google2.fda.gov/search?q=clonidine&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20FTIMD%20and%20synthesis)]

[^11^C]FTIMD was synthesized remotely via a reaction of [^11^C]methyl iodine (produced from [^11^C]CO_2_) with the tributylstannyl precursor in the presence of tris(dibenzylideneacetone)dipalladium(0) and tri(O-tolyl)phosphine in dimethylformamide for 5 min at 130°C (15). [^11^C]FTIMD was purified with high-performance liquid chromatography, with a radiochemical yield of 5.4 ± 2.0% (n = 7) from [^11^C]CO_2_ at end of bombardment (EOB). The radiochemical purity was >95%, and the specific activity was 108 ± 33 GBq/μmol (2.9 ± 0.9 Ci/μmol) at end of synthesis (EOS). Total time of synthesis was 30 min from EOB. To prepare [^11^C]FTIMD with ultra-high specific activity (4,470 ± 1,660 GBq/μmol (120 ± 45 Ci/μmol) at EOS), [^11^C]methyl iodine (produced from iodination of [^11^C]methane) was used with (n = 11) (16). The cLogD (pH 7.4) value for FTIMD was 1.42.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20FTIMD%20and%20in%20vitro)]

On the basis of in vitro competition binding studies, Anastassiadou et al. (14) reported inhibition constant (K_i_) values for FTIMD of 3.0 nM for I_2_R, >10,000 nM for I_1_R, >10,000 nM for α_1_-adrenoceptor, and >10,000 nM for α_2_-adrenoceptor.

In an in vitro autoradiography study, the distribution pattern of [¹¹C]FTIMD (200 nM) in the monkey brain was studied (17). The rank order of radioactivity was caudate > hippocampus > globus pallidus > putamen > amygdala > thalamus > cortex > cerebellum, which was similar to that of [³H]idazoxan binging to I₂R sites in the human brain (12). The specific binding of [¹¹C]FTIMD accounted for >97% of total binding in the brain regions expressing I₂R using 10,000 nM FTIMD and BU224 as I_2_R inhibitor ligands.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20FTIMD%20and%20rodentia)]

Ex vivo biodistribution of 11–20 MBq (0.30–0.54 mCi) [^11^C]FTIMD was studied in normal rats (n = 4/group) at 5, 15, and 30 min after injection (15). The tissue with the highest accumulation (standard uptake value) at 5 min after injection was the kidney (12.20), followed by the lung (4.35), brain (2.51), liver (2.49), small intestine (2.29), spleen (2.12), pancreas (2.08), heart (1.22), muscle (1.17), and blood (0.38). Most tissues showed moderate to rapid washout, except for the liver, which showed a gradual increase. The brain/blood ratio at 15 min after injection was 7.0. Co-injection of FTIMD (1 mg/kg) reduced the brain accumulation and brain/blood ratio by 22% and 32% (P < 0.05), respectively. Co-injection of another I_2_R inhibitor BU224 (1 mg/kg) reduced the brain accumulation and brain/blood ratio by 21% and 33% (P < 0.05), respectively. On the other hand, co-injection of I_1_R/α_2_-adrenoceptor ligands moxonidine (1 mg/kg) and efaroxan (1 mg/kg) showed little effect on the brain accumulation and brain/blood ratio. [^11^C]FTIMD remained >98% intact in the brain at 15 min and 30 min after injection, whereas only 57% and 37% remained intact in the plasma at 15 min and 30 min after injection, respectively. In a separate study in mice, specific accumulation of [^11^C]FTIMD was observed in the liver and pancreas (18).

Kawamura et al. (15) performed dynamic PET scans in four rats (46–117 MBq, 1.24–3.16 mCi) for 60 min after injection of [^11^C]FTIMD. High levels of radioactivity were detected in the arcuate nucleus, interpeduncular nucleus, hippocampus, and ependymal cell layer. Pretreatment with BU224 (1 mg/kg, 5 min) reduced radioactivity across the brain regions. Multilinear analysis showed a better fit than one- and two-compartment analysis. Regions of analysis showed the highest distribution volume (V_T_) values in the ependymal cell layer (15.09), followed by the hippocampus (14.24), cortex (13.85), arcuate nucleus (13.54), interpeduncular nucleus (12.87), and cerebellum (10.90). Pretreatment with BU224 (1 mg/kg, 5 min) reduced the V_T_ values by 17%–34%. Using [^11^C]FTIMD with ultra-high specific activity, the V_T_ values (13.77–19.02) were higher than those of [^11^C]FTIMD (10.90-15.09) with normal specific activity (16). Pretreatment with BU224 reduced the V_T_ values by 29%–45%, which were significantly higher than those of [^11^C]FTIMD with normal specific activity (P < 0.05).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20FTIMD%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=FTIMD%20and%20primate)]

In PET studies, 160 MBq (4.3 mCi) [^11^C]FTIMD (1.26 nmol) was intravenously injected into a conscious male monkey (17). The radioactivity was accumulated in the thalamus, arcuate nucleus, cingulate cortex, occipital cortex, hippocampus, striatum, cerebellum, and frontal cortex. Pretreatment with BU224 (5 mg/kg, 5 min) reduced the accumulated radioactivity to approximately 66%–75% of the baseline measurement at 15–45 min after injection of [¹¹C]FTIMD.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20FTIMD%20and%20human)]

No publications are currently available.

## References

1 Michel M.C., Ernsberger P. (1992). Keeping an eye on the I site: imidazoline-preferring receptors. Trends Pharmacol Sci.
2 Hamilton C.A. (1995). Imidazoline receptors, subclassification, and drug-induced regulation. Ann N Y Acad Sci.
3 El-Ayoubi R., Gutkowska J., Regunathan S., Mukaddam-Daher S. (2002). Imidazoline receptors in the heart: characterization, distribution, and regulation. J Cardiovasc Pharmacol.
4 Ernsberger P., Graves M.E., Graff L.M., Zakieh N., Nguyen P., Collins L.A., Westbrooks K.L., Johnson G.G. (1995). I1-imidazoline receptors. Definition, characterization, distribution, and transmembrane signaling. Ann N Y Acad Sci.
5 Ruggiero D.A., Regunathan S., Wang H., Milner T.A., Reis D.J. (1995). Distribution of imidazoline receptor binding protein in the central nervous system. Ann N Y Acad Sci.
6 Lanier S.M., Ivkovic B., Singh I., Neumeyer J.L., Bakthavachalam V. (1993). Visualization of multiple imidazoline/guanidinium-receptive sites. J Biol Chem.
7 Nikolic, K. and D. Agbaba, Imidazoline Antihypertensive Drugs: Selective I(1) -Imidazoline Receptors Activation. Cardiovasc Ther, 2011
8 Piletz J.E., Zhu H., Ordway G., Stockmeier C., Dilly G., Reis D., Halaris A. (2000). Imidazoline receptor proteins are decreased in the hippocampus of individuals with major depression. Biol Psychiatry.
9 Garcia-Sevilla J.A., Escriba P.V., Walzer C., Bouras C., Guimon J. (1998). Imidazoline receptor proteins in brains of patients with Alzheimer's disease. Neurosci Lett.
10 Reynolds G.P., Boulton R.M., Pearson S.J., Hudson A.L., Nutt D.J. (1996). Imidazoline binding sites in Huntington's and Parkinson's disease putamen. Eur J Pharmacol.
11 Martin-Gomez J.I., Ruiz J., Callado L.F., Garibi J.M., Aguinaco L., Barturen F., Javier Meana J. (1996). Increased density of I2-imidazoline receptors in human glioblastomas. Neuroreport.
12 De Vos H., Bricca G., De Keyser J., De Backer J.P., Bousquet P., Vauquelin G. (1994). Imidazoline receptors, non-adrenergic idazoxan binding sites and alpha 2-adrenoceptors in the human central nervous system. Neuroscience.
13 Tesson F., Prip-Buus C., Lemoine A., Pegorier J.P., Parini A. (1991). Subcellular distribution of imidazoline-guanidinium-receptive sites in human and rabbit liver. Major localization to the mitochondrial outer membrane. J Biol Chem.
14 Anastassiadou M., Danoun S., Crane L., Baziard-Mouysset G., Payard M., Caignard D.H., Rettori M.C., Renard P. (2001). Synthesis and pharmacological evaluation of imidazoline sites I1 and I2 selective ligands. Bioorg Med Chem.
15 Kawamura K., Naganawa M., Konno F., Yui J., Wakizaka H., Yamasaki T., Yanamoto K., Hatori A., Takei M., Yoshida Y., Sakaguchi K., Fukumura T., Kimura Y., Zhang M.R. (2010). Imaging of I2-imidazoline receptors by small-animal PET using 2-(3-fluoro-[4-11C]tolyl)-4,5-dihydro-1H-imidazole ([11C]FTIMD). Nucl Med Biol.
16 Kawamura K., Kimura Y., Yui J., Wakizaka H., Yamasaki T., Hatori A., Kumata K., Fujinaga M., Yoshida Y., Ogawa M., Nengaki N., Fukumura T., Zhang M.R. (2012). PET study using [(11)C]FTIMD with ultra-high specific activity to evaluate I(2)-imidazoline receptors binding in rat brains. Nucl Med Biol.
17 Kawamura K., Maeda J., Hatori A., Okauchi T., Nagai Y., Higuchi M., Suhara T., Fukumura T., Zhang M.R. (2011). In vivo and in vitro imaging of I imidazoline receptors in the monkey brain. Synapse.
18 Kawamura K., Yui J., Konno F., Yamasaki T., Hatori A., Wakizaka H., Fujinaga M., Kumata K., Yoshida Y., Ogawa M., Nengaki N., Yanamoto K., Fukumura T., Zhang M.R. (2012). Synthesis and evaluation of PET probes for the imaging of I2 imidazoline receptors in peripheral tissues. Nucl Med Biol.